# ^18^F-Labeled N-(4-(6,7-dimethoxy-3,4-dihydroisoquinolin-2(1H)-yl)butyl)-2-(2-fluoroethoxy)-5-methylbenzamide

Chemical name: | ^18^F-Labeled N-(4-(6,7-dimethoxy-3,4-dihydroisoquinolin-2(1H)-yl)butyl)-2-(2-fluoroethoxy)-5-methylbenzamide | [image]
Abbreviated name: | [^18^F]3c | [image]
Synonym: | | [image]
Agent Category: | Compound | [image]
Target: | Sigma-2 receptor | [image]
Target Category: | Receptor | [image]
Method of detection: | Positron emission tomography (PET) | [image]
Source of signal / contrast: | ^18^F | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structure of [^18^F]3c.

## Background

[PubMed] (http://www.ncbi.nlm.nih.gov/pubmed?term=sigma%202%20receptor&cmd=DetailsSearch)

Sigma receptor (SR) subtypes 1 (Sig-1R) and 2 (Sig-2R) and are known to be present primarily in the central nervous system and the peripheral tissues. Both receptor subtypes have a different distribution in the two types of tissues, and the exact biological function of these receptors is not known (1). Of the two receptor subtypes, only the Sig-1R has been cloned, expressed, and purified (2). The Sig-2R is known to be overexpressed in various malignant tumors and is believed to promote cell proliferation, indicating that these receptors may play a role in the development of some cancers (3). As a consequence, the Sig-2R have been suggested to be biomarkers for tumor cell proliferation (4) and could be targeted for the development of different anti-cancer drugs (5) or imaging agents for tumors that overexpress Sig-2R (3, 5). Several clinical trials (http://clinicaltrials.gov/ct2/results?term=sigma+2+receptor) have been approved by the United States Food and Drug Administration for the evaluation of drugs that target the Sig-2R for the imaging and treatment of different clinical conditions. In addition, Sig-2R ligands have been used in preclinical studies to chemosensitize (http://mct.aacrjournals.org/content/2/8/805.full.pdf+html) tumors to low doses of anti-cancer drugs that are otherwise toxic when given at high doses to animals bearing mammalian cell line tumors (6, 7).

Investigators have developed and characterized several SR ligands, but most of them are either selective only for the Sig-1R or have similar affinity for both SR subtypes, therefore limiting their use as anti-cancer drugs that target the Sig-2R or as detection and imaging agents for this receptor (3, 7). In an effort to develop a ligand with high specificity for Sig-2R, Tu et al. synthesized a series of ^18^F-labeled benzamide analogs and evaluated these radiolabeled compounds with positron emission tomography (PET) and computed tomography (CT) imaging of mice bearing allograft tumors expressing the receptor (3). Among the various compounds tested, N-(4-(6,7-dimethoxy-3,4-dihydroisoquinolin-2(1H)-yl)butyl)-2-(2-[^18^F]-fluoroethoxy)-5-methylbenzamide (designated [^18^F]3c) and another analog, N-(4-(6,7-dimethoxy-3,4-dihydroisoquinolin-2(1H)-yl)butyl)-2-(2-[^18^F]-fluoroethoxy)-5-iodo-3-methoxybenzamide (designated [^18^F]3f), were determined to be most suitable for the detection of solid tumors expressing Sig-2R with the use of PET and CT imaging. This chapter describes the in vitro characterization and in vivo biodistribution of [^18^F]3c and the PET/CT imaging with [^18^F]3c. The in vitro and in vivo characterization of [^18^F]3f are described in a separate chapter in MICAD (www.micad.nih.gov) (8).

### Other sources of information regarding SRs

Other SR imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=sigma+receptor++AND+micad%5Bbook%5D&doptcmdl=TOCView&log%24=booksrch&bname=micad).

Sigma receptors in OMIM (http://www.ncbi.nlm.nih.gov/omim?term=sigma%20receptors) (Online Mendelian Inheritance in Man).

Protein sequences of human SR1, isoform1 (http://www.ncbi.nlm.nih.gov/protein/NP_005857.1?ordinalpos=3&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum) and isoform 2 (http://www.ncbi.nlm.nih.gov/protein/NP_671513.1?ordinalpos=2&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum).

Nucleotide (mRNA) sequences of SR1, variant 1 (http://www.ncbi.nlm.nih.gov/nuccore/NM_005866.2?ordinalpos=4&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum) and variant 2 (http://www.ncbi.nlm.nih.gov/nuccore/NM_147157.1?ordinalpos=3&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-3c%5BAll%20Fields%5D%20AND%20%28%22metabolism%22%5BMeSH%20Terms%5D%20OR%20%22metabolism%22%5BAll%20Fields%5D%20OR%20%22synthesis%22%5BAll%20Fields%5D%29&cmd=DetailsSearch&log$=details)]

The synthesis and ^18^F-labeling of 3c has been described by Tu et al. (3). The total time of synthesis to obtain [^18^F]3c was ~2 h with a decay-corrected yield of ~35%. The radiochemical purity of the labeled compound was >99% as determined with analytical high-performance liquid chromatography with a specific activity of >74.07 TBq/mmol (2,000 Ci/mmol). The entire procedure, including purification, was completed in approximately 2 h. The stability and conditions used to store [^18^F]3c were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-3c%20in%20vitro&cmd=DetailsSearch)]

In vitro receptor binding studies with [^18^F]3c were performed by Tu et al. (3) using membranes isolated from liver homogenates as described elsewhere (9). The affinity of 3c for the two SR subtypes was determined by competition studies using [^3^H](+)-pentazocine (for Sig-1R) and [^3^H]1,3-di(2-tolyl)guanidine in the presence of unlabeled (+)-pentazocine (for Sig-2R). The affinity of 3c, as determined with Scatchard plot analysis, was reported to be 330 ± 25 and 6.95± 1.63 nM for Sig-1R and Sig-2R, respectively, with a Sig-1R/Sig-2R ratio of 48. For comparison, the affinity of 3f was reported to be 2,150 ± 410 and 0.26 ± 0.07 nM, respectively for the two receptor subtypes, with a Sig-1R/Sig-2R ratio of 8,190.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-3c%20rodentia&cmd=DetailsSearch)]

Tu et al. studied the biodistribution of [^18^F]3c in BALB/c mice bearing mouse mammary adenocarcinoma EMT-6 cell (these cells express high levels of the SRs (10)) tumors (3). The animals were injected with the labeled compound through the tail vein and euthanized at predetermined time points up to 120 min after the treatment (the number of animals used per time point was not indicated). After euthanasia, tissues from major organs of the animals were removed, weighed, and counted for accumulated radioactivity, and the data were presented as a percentage of injected dose per gram tissue (% ID/g). At 5 min after injection, maximum uptake of radioactivity was noticed in the kidneys (29.18 ± 1.92% ID/g) followed by the liver (23.33 ± 4.22% ID/g) and lungs (10.26 ± 0.71% ID/g). In comparison, the tumor had an uptake of 3.67 ± 0.45% ID/g at this time point. By 2 h after injection, the amount of label in the kidney, liver, lungs, and tumor tissues was reduced to 0.87 ± 0.13, 2.05 ± 0.43, 0.43 ± 0.07, and 0.64 ± 0.10% ID/g, respectively. A similar trend was noticed for the uptake of [^18^F]3f in all the tissues, including the tumors. The tumor/muscle (T/M) and tumor/fat (T/F) ratios for [^18^F]3c were ~3 and ~8, respectively, at 2 h after injection. For [^18^F]3f, the T/M and T/F ratios were ~7 and ~6, respectively. Both [^18^F]3c and [^18^F]3f were reported to have rapid clearance from blood, indicating that both tracers were probably suitable for the detection and imaging of solid tumors expressing Sig-2R.

For blocking studies, mice were injected with [^18^F]3c in presence of excess (1 mg/Kg) unlabeled N-(4-fluorobenzyl)piperidinyl-4-(3-bromophenyl) acetamide, which has a high affinity for the two SR subtypes (3), and the mice were euthanized 1 h after the treatment (the number of animals used was not reported) (3). Under these conditions, the T/M and T/F ratios for this labeled compound were reduced by ~50%, indicating that the radiochemical bound selectively to the Sig-2R. Similar results were obtained with [^18^F]3f under these experimental conditions.

Mice bearing EMT-6 cell tumors were injected with [^18^F]3c as detailed above, and PET/CT imaging was performed on the animals 1 h later (3). Both detection methods were reported to identify the tumors in the animals easily. Similar results were reported when [^18^F]3f was used as an imaging agent.

On the basis of the results obtained from these studies, the investigators concluded that both [^18^F]3c and [^18^F]3f were equally suitable for the detection and imaging of solid tumors expressing Sig-2R using PET (3).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-3c%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-3c%20Non-Human%20Primates&cmd=DetailsSearch)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-3c%20Human%20Studies&cmd=DetailsSearch)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

Some studies reported in this chapter were supported by National Institutes of Health grants CA-102869 and P41RR0954.

## References

1 Collier T.L., Waterhouse R.N., Kassiou M. (2007). Imaging sigma receptors: applications in drug development. Curr Pharm Des.
2 Hanner M., Moebius F.F., Flandorfer A., Knaus H.G., Striessnig J., Kempner E., Glossmann H. (1996). Purification, molecular cloning, and expression of the mammalian sigma1-binding site. Proc Natl Acad Sci U S A.
3 Tu Z., Xu J., Jones L.A., Li S., Dumstorff C., Vangveravong S., Chen D.L., Wheeler K.T., Welch M.J., Mach R.H. (2007). Fluorine-18-labeled benzamide analogues for imaging the sigma2 receptor status of solid tumors with positron emission tomography. J Med Chem.
4 Wheeler K.T., Wang L.M., Wallen C.A., Childers S.R., Cline J.M., Keng P.C., Mach R.H. (2000). Sigma-2 receptors as a biomarker of proliferation in solid tumours. Br J Cancer.
5 Hashimoto K., Ishiwata K. (2006). Sigma receptor ligands: possible application as therapeutic drugs and as radiopharmaceuticals. Curr Pharm Des.
6 Kashiwagi H., McDunn J.E., Simon P.O., Goedegebuure P.S., Vangveravong S., Chang K., Hotchkiss R.S., Mach R.H., Hawkins W.G. (2009). Sigma-2 receptor ligands potentiate conventional chemotherapies and improve survival in models of pancreatic adenocarcinoma. J Transl Med.
7 Chu W., Xu J., Zhou D., Zhang F., Jones L.A., Wheeler K.T., Mach R.H. (2009). New N-substituted 9-azabicyclo[3.3.1]nonan-3alpha-yl phenylcarbamate analogs as sigma2 receptor ligands: synthesis, in vitro characterization, and evaluation as PET imaging and chemosensitization agents. Bioorg Med Chem.
8 Chopra, A., [18F]Labeled N-(4-(6,7-dimethoxy-3,4-dihydroisoquinolin-2(1H)-yl)butyl)-2-(2-fluoroethoxy)-5-iodo-3-methoxybenzamide ([18F]3f). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
9 Xu J., Tu Z., Jones L.A., Vangveravong S., Wheeler K.T., Mach R.H. (2005). [3H]N-[4-(3,4-dihydro-6,7-dimethoxyisoquinolin-2(1H)-yl)butyl]-2-methoxy-5 -methylbenzamide: a novel sigma-2 receptor probe. Eur J Pharmacol.
10 Colabufo N.A., Berardi F., Contino M., Fazio F., Matarrese M., Moresco R.M., Niso M., Perrone R., Tortorella V. (2005). Distribution of sigma receptors in EMT-6 cells: preliminary biological evaluation of PB167 and potential for in-vivo PET. J Pharm Pharmacol.